# 1-(2,4-Dichlorophenyl)-5-(4-[^123^I]iodophenyl)-4-methyl-1H-pyrazole-3-carboxylic acid N',N'-dimethyl-hydrazide

Chemical name: | 1-(2,4-Dichlorophenyl)-5-(4-[^123^I]iodophenyl)-4-methyl-1H-pyrazole-3-carboxylic acid N',N'-dimethyl-hydrazide
Abbreviated name: | [^123^I]Me_2_Pyr
Synonym:
Agent category: | Compound
Target: | Cannabinoid CB1 receptors
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and some peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominantly in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. The CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid that is found in marijuana and activates CB1 receptors (7). THC has a very high lipophilicity (log D_7.4_ value of 7), which causes imaging studies using radiolabeled THC to be unsuccessful because of slow entry into the brain and high nonspecific binding in the brain. However, a high lipophilicity is essential for binding to CB1 receptors, and an optimal lipophilicity (log D_7.4_ 1–4) is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2, which also exhibit high nonspecific binding and lipophilicity, limiting their application in imaging (8). Therefore, there is a need to lower the lipophilicity of the CB1 radioligands with little effect on binding affinity and ability to cross the BBB. 1-(2,4-Dichlorophenyl)-5-(4-[^123^I]iodophenyl)-4-methyl-1H-pyrazole-3-carboxylic acid N',N'-dimethyl-hydrazide ([^123^I]Me_2_Pyr) is a CB1 analog of N-(morpholin-4-yl)-5-(4-[^123^I]iodophenyl)-1-(2,4-dichlorophenyl)-4-methyl-1H-pyrazole-3-carboxamide ([^123^I]AM281 (http://www.ncbi.nlm.nih.gov/books/NBK24613/)) with the N-heterocyclic residue substituted by a dimethylamino group (9). [^123^I]Me_2_Pyr is being developed as a single-photon emission computed tomography (SPECT) agent for the non-invasive study of CB1 receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (CB1 receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=CB1+AND+micad%5Bbook%5D))
- Gene information in NCBI (CB1 receptors (http://www.ncbi.nlm.nih.gov/gene/1268))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CB1 receptors (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=114610))
- Clinical trials (CB1 receptors (http://www.clinicaltrials.gov/ct2/results?term=CB1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20synthesis)]

Gielow et al. (9) reported synthesis of [^123^I]Me_2_Pyr by radioiododestannylation reaction of the tributyltin precursor with [^123^I]iodide in the presence of HCl and chloramine-T. Radiochemical yields were 48% after high-performance liquid chromatography purification. Specific activities were >75 GBq/μmol (>2 Ci/μmol) with a radiochemical purity of >92%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20in%20vitro)]

Gielow et al. (9) reported that the lipophilicity values were 3.7 for AM281, 4.5 for Me_2_Pyr, and 4.8 for SR141716A.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20rodentia)]

Ex vivo autoradiography of rat brain showed the highest radioactivity in the substantia nigra, globus pallidus, and cerebellum at 120 min after injection of [^125^I]AM281 (n = 3) or [^125^I]Me_2_Pyr (n = 2), which is consistent with the CB1 distribution in the brain (9). Ratios of [^125^I]AM281 in the substantia nigra/frontal cortex, globus pallidus/frontal cortex, and cerebellum/frontal cortex were 1.72, 1.68, and 1.30, respectively; ratios of [^125^I]Me_2_Pyr in the substantia nigra/frontal cortex, globus pallidus/frontal cortex, and cerebellum/frontal cortex were 1.89, 1.67, and 1.46, respectively. However, these ratios were not different between the two compounds.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20%28primate%20not%20human%29)]

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20Me2Pyr%20and%20human)]

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Gielow P., Klinge P., Knapp W.H., Berding G. (2006). Synthesis and preliminary biological evaluation of [123I]Me2Pyr, a new potential ligand for imaging of central cannabinoid CB1 receptors. Appl Radiat Isot.